# N-(2-(Diethylamino)ethyl)-6-[^18^F]fluoronicotinamide

Chemical name: | N-(2-(Diethylamino)ethyl)-6-[^18^F]fluoronicotinamide
Abbreviated name: | [^18^F]2
Synonym:
Agent category: | Compound
Target: | Melanin
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide)]

Malignant melanoma is the sixth most common cancer in the United States with ~130,000 cases/yr (1). Early diagnosis and prompt surgical removal comprise the best approach for a possible cure because malignant melanoma is a very aggressive cancer (2). Melanomas develop from activated or genetically altered neoplastic melanocytes that contain melanin (3-5). Melanin pigment is synthesized and deposited within melanosomes (6). Eumelanin and pheomelanin are the two major types of melanin. Eumelanin is the predominant melanin pigment found in primary tumors. Pheomelanin tends to associate with progression of the disease. Melanins are complex, negatively charged molecules with hydrophobic surfaces, and they have the capability to bind many different types of compounds (3). Therefore, melanins represent a very attractive target for both diagnosis and treatment.

Benzamide (BZA) derivatives and iodobenzamides have been found to have affinity for melanomas (3, 7-9). The exact mechanisms of uptake of these compounds have not been fully established (7, 10, 11). Direct melanin binding, involvement in the melanin biosynthesis pathway, and sigma (σ) receptor mediation have been proposed as the most likely mechanisms for different compounds. In addition, available vascular concentrations of these compounds and their ability to transport into the melanoma cells also influence their cellular uptake (11). Melanin-targeting radiopharmaceuticals that are based on BZA such as [^123^I]BZA, [^123^I]BZA_2_, and [^123^I]IBZM have been investigated and developed for molecular imaging of malignant melanomas (12-14). To produce a positron emission tomography (PET) probe with higher tumor uptake and faster body clearance, Greguric et al. (15) designed and prepared N-(2-(diethylamino)ethyl)-6-[^18^F]fluoronicotinamide ([^18^F] 2), which has an alkylpiperazinyl moiety. Their study showed that [^18^F]2 has a high selective uptake in the murine B16F0 melanoma tumor, and the uptake was most likely related to melanin binding.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Melanin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Melanin (http://www.ncbi.nlm.nih.gov/gene/5367))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=melanin)
- Information about N-(2-(diethylamino)ethyl)-6-[^18^F]fluoronicotinamide in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=search&db=pcsubstance&term=85756802)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide%20and%20synthesis)]

Greguric et al. (15) reported the synthesis of [^18^F]2 by a one-step direct [^18^F]fluorination of the chloronicotinamide precursor in the presence of K[^18^F]K2.2.2 complex. The reaction was stirred and heated at 150°C for 5 min. [^18^F]2 was purified with high performance liquid chromatography (HPLC) with a radiochemical purity of >99% and a nondecay corrected specific activity of >150 GBq/µmol (4.1 Ci/µmol) at the end of synthesis. Lipophilicity of [^18^F]2 was 1.1 (log P_7.5_) as determined by HPLC. [^18^F]2 was > 98% intact in saline for 3-4 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide%20and%20rodentia)]

Greguric et al. (15) performed biodistribution studies in black mice (n = 5/group) bearing murine melanotic B-16F0 after intravenous injection of 0.37-0.74 MBq (10-20 μCi) [^18^F]2. There was high tumor radioactivity accumulation, low normal organ radioactivity accumulation, and rapid body clearance. The tumor radioactivity levels in percentage injected dose per gram (% ID/g) were 7.0 ± 0.9 (0.25 h), 8.4 ± 1.5 (1 h), 9.4 ± 1.6 (2 h), 7.8 ± 1.4 (3 h), and 7.7 ± 2.3 (6 h). At 1 h, the radioactivity levels (% ID/g) in other major organs were 19 (eye), 3.4 (stomach), 3.3 (thyroid), 2.4 (spleen), 1.6 (lung), and 1.4 (bone). At 6 h, these levels (% ID/g) decreased to 16 (eye), 0.19 (stomach), 0.17 (thyroid), 0.47 (spleen), 0.07 (lung), and 0.52 (bone). HPLC analysis showed that 70% of the radioactivity in the plasma and >90% of the radioactivity in the tumor, eye and urine represented intact [^18^F]2 at 2 h after injection. In comparison, the tumor and eye radioactivity levels (n = 5) were very low with ~1% ID/g (1 h) and ~0.1% ID/g (6 h) in nude mice bearing A375 human amelanotic melanoma tumors. Whole-body PET imaging was performed in mice bearing B16F0 melanotic tumor. A dose of 27 MBq (0.7 mCi) [^18^F]2 was administered by intravenous injection, and images were obtained at 1 h after injection. The results showed that the tumor and urinary bladder had the highest tumor radioactivity level. The eyes were visualized with lower radioactivity level. No blocking experiment was performed in this preliminary study.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoronicotinamide%20and%20human)]

No publication is currently available.

## References

1 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Dadachova E., Casadevall A. (2005). Melanin as a potential target for radionuclide therapy of metastatic melanoma. Future Oncol.
4 Cohen-Solal K.A., Crespo-Carbone S.M., Namkoong J., Mackason K.R., Roberts K.G., Reuhl K.R., Chen S. (2002). Progressive appearance of pigmentation in amelanotic melanoma lesions. Pigment Cell Res.
5 Sulaimon S.S., Kitchell B.E. (2003). The biology of melanocytes. Vet Dermatol.
6 Hearing V.J. (2000). The melanosome: the perfect model for cellular responses to the environment. Pigment Cell Res.
7 Pham, T.Q., P. Berghofer, X. Liu, I. Greguric, B. Dikic, P. Ballantyne, F. Mattner, V. Nguyen, C. Loc'h, and A. Katsifis, Preparation and Biologic Evaluation of a Novel Radioiodinated Benzylpiperazine, 123I-MEL037, for Malignant Melanoma. J Nucl Med, 2007
8 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
9 Wolf M., Bauder-Wust U., Mohammed A., Schonsiegel F., Mier W., Haberkorn U., Eisenhut M. (2004). Alkylating benzamides with melanoma cytotoxicity. Melanoma Res.
10 Dittmann H., Coenen H.H., Zolzer F., Dutschka K., Brandau W., Streffer C. (1999). In vitro studies on the cellular uptake of melanoma imaging aminoalkyl-iodobenzamide derivatives (ABA). Nucl Med Biol.
11 Eisenhut M., Hull W.E., Mohammed A., Mier W., Lay D., Just W., Gorgas K., Lehmann W.D., Haberkorn U. (2000). Radioiodinated N-(2-diethylaminoethyl)benzamide derivatives with high melanoma uptake: structure-affinity relationships, metabolic fate, and intracellular localization. J Med Chem.
12 Brandau W., Niehoff T., Pulawski P., Jonas M., Dutschka K., Sciuk J., Coenen H.H., Schober O. (1996). Structure distribution relationship of iodine-123-iodobenzamides as tracers for the detection of melanotic melanoma. J Nucl Med.
13 Moins N., D'Incan M., Bonafous J., Bacin F., Labarre P., Moreau M.F., Mestas D., Noirault E., Chossat F., Berthommier E., Papon J., Bayle M., Souteyrand P., Madelmont J.C., Veyre A. (2002). 123I-N-(2-diethylaminoethyl)-2-iodobenzamide: a potential imaging agent for cutaneous melanoma staging. Eur J Nucl Med Mol Imaging.
14 Salopek T.G., Scott J.R., Joshua A.V., Smylie M., Logus J.W., Morin C.A., McEwan A.J. (2001). Radioiodinated N-[3-(4-morpholino)propyl]-N-methyl-2-hydroxy-5-iodo-3-methylbenzylamine (ERC9): a new potential melanoma imaging agent. Eur J Nucl Med.
15 Greguric I., Taylor S.R., Denoyer D., Ballantyne P., Berghofer P., Roselt P., Pham T.Q., Mattner F., Bourdier T., Neels O.C., Dorow D.S., Loc'h C., Hicks R.J., Katsifis A. (2009). Discovery of [18F]N-(2-(diethylamino)ethyl)-6-fluoronicotinamide: a melanoma positron emission tomography imaging radiotracer with high tumor to body contrast ratio and rapid renal clearance. J Med Chem.